# ^99m^Tc-Labeled tumor-associated glycoprotein 72 binding peptides G3-15 and T3-15

Chemical name: | ^99m^Tc-Labeled tumor-associated glycoprotein 72 binding peptides G3-15 and T3-15
Abbreviated name: | [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15
Synonym:
Agent Category: | Peptides
Target: | Tumor-associated glycoprotein 72 (TAG-72)
Target Category: | Other (glycoprotein)
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72&cmd=DetailsSearch)]

The tumor-associated glycoprotein 72 (TAG-72) is a high molecular weight mucigenous protein that is found mainly in the extracellular matrix of neoplastic tumors (1). This glycoprotein is usually not expressed in normal tissues but is overexpressed in the tumors of several cancers, such as those of the colon and rectum (colorectal cancer), stomach, pancreas, ovaries, prostate, lung, breast, etc. Therefore, TAG-72 is considered to have much theranostic value (useful for the diagnosis and/or therapy of a disease) because it can be used for antigen-directed surgical resection of cancerous tumors with radiolabeled anti-TAG-72 monoclonal antibodies (mAb) (1). In addition, the detection or absence of TAG-72 expression in colorectal cancer tumors was shown to have prognostic value because individuals who had complete removal of tumors with surgery guided by mouse anti-Tag-72 mAb were shown to have a long-term survival advantage compared to patients who had an incomplete removal of the lesions (2). However, the main limitation of using radiolabeled antibodies (Ab) or their fragments to detect and treat malignant tumors is the long circulation half-life of these molecules and the development of human anti-mouse antibodies in the patients (3). In comparison, synthetic anti-tumor peptides that can be used for the noninvasive imaging and therapy of cancers show rapid clearance from circulation and non-target tissue, have more access and deeper penetration into the lesions, and may not be immunogenic (3-5).

Recently, the peptides GGVSCMQTSPVCENNL (A2-6) and NPGTCKDKWEICLLNGG (A3-10) were identified from a phase-display peptide library (f88-4/cys6) against TAG-72 and labeled with ^99m^Tc to generate [^99m^Tc]-A2-6 and [^99m^Tc]-A3-10 (4). The labeled peptides were then evaluated in mice for the detection of LS-174T cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CL-188&Template=cellBiology) xenograft tumors that overexpress the TAG-72 antigen. In another study, two new peptides, FRERCDKHPQKCTKFL (G3-15) and DPRHCQKRVLPCPAWL (T3-15), which had a high affinity for the TAG-72 antigen, were identified when a modified procedure (from that used to purify the A2-6 and A3-10 peptides) was used to purify peptides from the f88-4/cys6 phage library (3). These peptides were then labeled with ^99m^Tc to obtain [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15, and the labeled compounds were tested for the detection of LS-174T cell xenograft tumors in mice. This chapter describes the results obtained with [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15. Studies performed with [^99m^Tc]-A2-6 and [^99m^Tc]-A3-10 are described in a separate chapter of MICAD (www.micad.nih.gov) (6).

### Related Resource Links

TAG-72 related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=TAG-72+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=TAG-72) related to TAG-72

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20TAG-72%20binding%20peptides&cmd=DetailsSearch)]

Peptides G3-15 and T3-15 were identified from the f88-4/cys6 phage peptide library by modifying a procedure used earlier to purify peptides from the phage library that bound the TAG-72 glycoprotein (4) as described by Xiao et al. (3). For studies described in this chapter, the new peptides were obtained from a commercial source in their native L-configuration, conjugated with N-hydroxysuccinimidyl-S-acetyl-mercaptoacetyltriglycine, and labeled with ^99m^Tc as described elsewhere (3). The labeled peptides were purified on a Bio-Rad P2 size-exclusion column and had a radiochemical purity of >90% as determined with reversed-phase high-performance liquid chromatography (RP-HPLC) (4). The number of metal chelating molecules conjugated to each peptide, radiochemical yield and specific activity of the labeled peptides were not reported.

The stability of [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15 was determined by incubating the labeled peptides in serum (source not reported) at 37°C for up to 60 min (3). A P2 column size-exclusion HPLC analysis of the peptides at 5 min into the incubation showed that both labeled peptides were intact, but HPLC analysis at 60 min revealed that ~5% of both ^99m^Tc-labeled peptides were bound to serum proteins as indicated by the appearance of two high molecular weight peaks in the HPLC chromatograms (3). The high molecular weight peaks observed with both tracers were not characterized.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20in%20vitro%20studies&cmd=DetailsSearch\)]

The IC_50_ values of [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15 were determined with an in vitro competitive binding assay (3). For this, LS-174T cells were incubated with the ^99m^Tc-labeled peptides in the presence of increasing concentrations (10−^13^ to 10−^4^ mol/L) of the respective non-labeled peptides, and the IC_50_ values were calculated as described by Chen et al. (4). The IC_50_ values of G3-15 and T3-15 were reported to be 10.32 nM and 0.29 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15 was investigated in nude mice (n = 4 animals/group) bearing LS-174T cell tumors on the left thigh (3). The animals were injected with either [^99m^Tc]-G3-15 or [^99m^Tc]-T3-15 through the tail vein. The animals were euthanized at 5, 30, and 90 min postinjection (p.i.) to remove all the major organs and determine the amount of radioactivity accumulated in the various tissues. Data were presented as percent of injected dose per gram tissue (% ID/g). Both labeled peptides had a similar pattern of biodistribution in the rodents. The kidneys showed the highest accumulation of label, with both tracers present at all the three time points. At 90 min p.i., most tissues had a radioactivity uptake of <1% ID/g. With [^99m^Tc]-G3-15, the uptake of radioactivity in the tumor decreased from 2.01 ± 0.16% ID/g at 5 min p.i. to 0.17 ± 0.04% ID/g at 90 min p.i. Similarly, with [^99m^Tc]-T3-15, tumor uptake of the tracer decreased from 2.56 ± 0.61% ID/g at 5 min p.i. to 0.45 ± 0.09% ID/g at 90 min p.i. The tumor/muscle (normal thigh) ratios with [^99m^Tc]-G3-15 and [^99m^Tc]-T3-15 increased from 1.10 and 1.02 at 5 min p.i., respectively, to 1.60 and 1.87, respectively at 90 min, p.i.

In another study, single-photon emission computed tomography (SPECT)/computed tomography (CT) whole-body scans were acquired at 20 min and 60 min p.i. from groups of mice (under anesthesia) injected with either [^99m^Tc]-G3-15 or [^99m^Tc]-T3-15 as described by Xiao et al. (3). SPECT/CT images acquired at 20 min p.i. showed that both tracers had cleared from circulation and that the tumor was clearly visible with both the labeled peptides. At this time point, maximum radioactivity was observed in the kidneys, with the radiolabeled compounds and some label present in the intestinal tract, gall bladder, and urinary bladder. At 60 min p.i., the tumor was visible only with [^99m^Tc]-T3-15, indicating that, compared to [^99m^Tc]-G3-15, this tracer had a higher affinity for the TAG-72 glycoprotein as observed during the in vitro studies (see above).

From these studies, the investigators concluded that, by using a modified purification procedure to purify peptides from the f88-4/cys6 phage peptide library, they could identify two new peptides, G3-15 and T3-15, which had a high affinity for the TAG-72 antigen (3). The investigators suggest that further development of these peptides may be useful to produce probes for the imaging and treatment of cancer in humans.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=TAG-72%20binding%20peptides%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No supplemental information is currently available.

## NIH Support

A part of the studies reported in this chapter were supported by a National Institutes of Health grant CA111606.

## References

1 Povoski S.P., Hatzaras I.S., Mojzisik C.M., Martin E.W. (2011). Oncologic theranostics: recognition of this concept in antigen-directed cancer therapy for colorectal cancer with anti-TAG-72 monoclonal antibodies. Expert Rev Mol Diagn.
2 Povoski, S.P., I.S. Hatzaras, C.M. Mojzisik, M.W. Arnold, G.H. Hinkle, C.L. Hitchcock, D.C. Young, and E.W. Martin, Jr., Antigen-Directed Cancer Surgery for Primary Colorectal Cancer: 15-Year Survival Analysis. Ann Surg Oncol, 2011
3 Xiao N., Cheng D., Wang Y., Chen L., Liu X., Dou S., Liu G., Liang M., Hnatowich D.J., Rusckowski M. (2011). Identification of a high affinity TAG-72 binding peptide by phage display selection. Cancer Biol Ther.
4 Chen L., Wang Y., Cheng D., Dou S., Liu X., Liu G., Hnatowich D.J., Rusckowski M. (2011). Comparing two TAG-72 binding peptides previously identified by phage display as potential imaging agents. Nucl Med Commun.
5 Rusckowski M., Gupta S., Liu G., Dou S., Hnatowich D.J. (2007). Evidence of specificity of radiolabeled phage display peptides for the TAG-72 antigen. Cancer Biother Radiopharm.
6 Chopra, A., 99mTc-Labeled tumor-associated glycoprotein 72 binding peptides, A2-6 and A3-10. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.